# DyLight 750-MES-1 E-selectin monoclonal antibody

Chemical name: | DyLight 750-MES-1 E-selectin monoclonal antibody
Abbreviated name: | DyLight 750-MES-1
Synonym:
Agent category: | Antibody
Target: | E-selectin
Target category: | Adhesion molecule
Method of detection: | Optical, near-infrared fluorescence (NIR)
Source of signal/contrast: | DyLight 750
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive complement to radionuclide imaging in small animals.

E-selectin is found on the cell surface of endothelial cells (4, 5). It binds to sialy-Lewis X (a carbohydrate moiety) on the cell surface of leukocytes. Tumor necrosis factor α (TNFα) and interleukin-1 (IL-1), released from inflammatory stimuli, upregulate E-selectin and other adhesion molecules expressed on the vascular endothelial cells, leading to leukocyte adhesion to the activated endothelium. E-selectin and other selectins are involved in arresting leukocytes on the endothelium for extravasation. An anti-E-selectin monoclonal antibody, MES-1, was conjugated with the NIR dye DyLight 750 to form DyLight 750-MES-1 for noninvasive NIR imaging of E-selectin expression in inflammation (6).

### Related Resource Links:

- Chapters in MICAD (E-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (E-selectin (http://www.ncbi.nlm.nih.gov/gene/6401)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (E-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D))
- Clinical trials (E-selectin (http://www.clinicaltrials.gov/ct2/results?term=E-selectin))
- Drug information in FDA (E-selectin (http://google2.fda.gov/search?q=e-selectin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR%20and%20synthesis)]

MES-1 was incubated with DyLight 750 N-hydroxysuccinimide ester for ~60 min at room temperature (6). DyLight 750-MES-1 was purified with column chromatography. Anti-DNP monoclonal antibody was also labeled with DyLight 750 as control (DyLight 750-IgG). There were 1.65 and 1.93 DyLight 750 molecules per MES-1 antibody and anti-DNP antibody, respectively. The dye/antibody ratios remained the same after dialysis, suggesting there were no free dye molecules. DyLight 750 dye has an excitation maximum at 752 nm and an emission maximum at 778 nm with an excitation efficiency of 210,000 M^-1^cm^-1^.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR%20and%20in%20vitro)]

Similar binding of DyLight 750-MES-1 and MES-1 to mouse E-selectin showed that there was no loss of immunoreactivity after labeling MES-1 with dye (6). There was >1-fold increase in fluorescence signal of DyLight 750-MES-1 binding to TNFα-activated mouse endothelial cells compared with untreated cells (P < 0.001). DyLight 750-IgG showed little binding to the activated cells or to the untreated cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR%20and%20rodentia)]

Gompels et al. (6) injected TNFα (50 ng) into the right hind paw to induce paw edema in mice as a model of inflammation. Maximal change in mean paw thickness was 0.4 mm at 4 h after injection. Immmunohistochemistry showed there was an increase in E-selectin expression in inflamed paws at 4 h but not at 24 h after injection of TNFα. Fluorescence imaging was performed at 0.5, 1, 2, 4, 8, and 24 h after intravenous injection of ~0.04 nmol DyLight 750-MES-1 (n = 5 mice) or DyLight 750-IgG (n = 5 mice). There was a progressive increase in mean fluorescence intensity (MFI) in inflamed paws from 0.5 h to 4 h, with peak MFI at 8 h after injection of DyLight 750-MES-1. However, no such increase was observed in the contralateral paws or in the inflamed paws of mice injected with DyLight 750-IgG. DyLight 750-MES-1 showed a 0.97-fold increase in MFI compared with DyLight 750-IgG in inflamed paws and a 1.46-fold increase compared with the contralateral paws (P < 0.001). In collagen-induced arthritis (CIA), DyLight 750-MES-1 showed a 1.34-fold increase in MFI relative to DyLight 750-IgG in arthritic paws (P < 0.01). There was a significant correlation between E-selectin expression and the severity of CIA (P < 0.01). Immmunohistochemistry showed a colocalization of E-selectin to microvessels within the inflamed synovium. Treatment with TNFα receptor:Fc fusion protein (binding to TNFα) abrogated the arthritis with a 50% reduction in the MFI of DyLight 750-MES-1.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=E-selectin%20NIR%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Bird M.I., Foster M.R., Priest R., Malhotra R. (1997). Selectins: physiological and pathophysiological roles. Biochem Soc Trans.
5 Rosen S.D., Bertozzi C.R. (1994). The selectins and their ligands. Curr Opin Cell Biol.
6 Gompels L.L., Madden L., Lim N.H., Inglis J.J., McConnell E., Vincent T.L., Haskard D.O., Paleolog E.M. (2011). In vivo fluorescence imaging of E-selectin: quantitative detection of endothelial activation in a mouse model of arthritis. Arthritis Rheum.